# 6-(3'-[^18^F]Fluoropropyl)-2-(4'-dimethylamino)phenylimidazol[1,2-α]pyridine

Chemical name: | 6-(3'-[^18^F]Fluoropropyl)-2-(4'-dimethylamino)phenylimidazol[1,2-α]pyridine
Abbreviated name: | [^18^F]FPPIP
Synonym:
Agent Category: | Compound
Target: | Amyloid-β (Aβ)
Target Category: | Specific binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DFPPIP%20OR%20FPPIP)]

6-(3'-[^18^F]Fluoropropyl)-2-(4'-dimethylaminophenylimidazol[1,2-α]pyridine ([^18^F]FPPIP) is a radioligand that was developed for positron emission tomography (PET) imaging of amyloid-β (Aβ) plaques in the central nervous system (CNS) for detection of Alzheimer’s disease (AD) (1). ^18^F is a positron emitter with a physical t_½_ of 109.7 min.

Aβ-peptide was sequenced from the meningeal blood vessels of AD patients and individuals with Downs syndrome (2). Aβ peptides contain 40−42 amino acid residues and are metabolic products of the Aβ precursor protein (APP) from cleavage by β- and γ-secretases (3). Aβ is also identified as the primary component of the neuritic plaques of AD patient brain tissue (4). The cloning of the gene that encodes the APP and its localization to chromosome 21 led to the hypothesis that Aβ accumulation is the primary event in AD pathogenesis (2, 5). This hypothesis proposes that neuronal death in AD is related to the toxic effect of Aβ on the adjacent cell bodies or cell processes (6). AD is a progressive, neurodegenerative disorders of the CNS, and is characterized by a common set of clinical and pathological features (3). In addition to Aβ, the microtubule-associated protein tau is also found in the cell body and axons of neurons as neurofibrillary tangles.

The search for a cure or effective treatment of AD requires in vivo detection and quantification of Aβ in the brain for evaluation of the efficacy of AD therapy (3). Various amyloid-imaging probes have been developed for PET, single-photon emission computed tomography, and optical imaging. These compounds generally have high binding affinity for amyloid fibrils and adequate permeability of blood−brain barrier (BBB) (7). Klunk et al. (8) studied [^11^C]6-OH-BTA-1 in AD patients and showed the potential usefulness of these probes. [^123^I]6-iodo-2(4'-N,N'-dimethylamino)phenylimidazol[1,2-α]pyridine ([^123^I]IMPY) has been reported as a potential SPECT agent for imaging Aβ plaques. Because PET can provide more accurate quantitative imaging, Zeng et al. (1) developed ^18^F-labeled IMPY analogs for PET imaging of AD plaques. [^18^F]FPPIP is produced by replacing the iodo group on IMPY with fluoropropyl.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFPPIP%20OR%20FPPIP%29%20AND%20synthesis)]

Zeng et al. (1) reported the synthesis of FPPIP from IMPY. IMPY was first prepared from condensation reaction between commercially available 2-amino-5-iodopyridine and 2-bromo-4'-dimethylaminoacetophenone in the presence of sodium bicarbonate as a mild base. IMPY was coupled with the tributyl(propylene)tin in toluene and palladium at 100ºC for 20 h to produce the corresponding intermediate alkene. This alkene was then converted to a hydroxyethyl compound by a hydroboration-oxidation reaction. FPPIP was finally produced by reaction of the hydroxyethyl compound with diethylaminosulfur trifluoride in methylene chloride at −78ºC to 23ºC for 2 h with a yield of 44%.

The radiosynthesis of [^18^F]FPPIP was accomplished by using the tosylate FPPIP precursor that was produced from reaction of FPPIP with tosylate chloride and triethylamine in methylene chloride at room temperature for 15 h with a yield of 52% (1). This precursor was then reacted with anhydrous ^18^F-labeled potassium fluoride and K_222_ in acetonitrile for 10 min at 90ºC. The entire radiolabeling procedure required 105 min from the end of bombardment. The decay-corrected yield was 51% and the radiochemical purity was >98%. The specific activity was 62.9−85.1GBq/μmol (1.7−2.3 Ci/μmol) at the time of injection.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFPPIP%20OR%20FPPIP%29%20AND%20in%20vitro)]

In vitro binding studies with unlabeled FPPIP were conducted with quantitative autoradiography by binding competition with [^125^I]IMPY in human AD cortical tissues (1). The inhibition constant (K_i_) was determined to be 48.3 nM. In comparison, IMPY had a K_i_ value of 10.3 nM. The lipophilicity coefficient log P (1-octanol and phosphate buffer at pH 7.4) of FPPIP was 2.84 whereas IMPY had a value of 3.58. The in vitro binding of [^18^F]FPPIP was shown in postmortem AD brain sections by autoradiography. Specific binding was found in cortical gray matter but not in the white matter. This specific binding was eliminated when the sections were pretreated with unlabeled FPPIP. No specific binding was found in normal brain sections. In a study that used in vitro Immunostaining with an Aβ-specific 4G8 monoclonal antibody, [^18^F]FPPIP labeling demonstrated a good correlation with Aβ plaque labeling by AG8 in the AD brain sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFPPIP%20OR%20FPPIP%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFPPIP%20OR%20FPPIP%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFPPIP%20OR%20FPPIP%29%20AND%20%28primate%20NOT%20human%29)]

Zeng et al. (1) performed PET imaging of [^18^F]FPPIP in a healthy rhesus monkey. The study showed easy brain entry and clearance from normal brain tissue. The peak standard uptake value of [^18^F]FPPIP was 1.6−2.7 at 9 min. Relatively fast nonspecific binding clearance was observed in cerebellum, frontal cortex, and subcortical white matter. No bone radioactivity was observed in the skull, which might indicate low in in vivo defluorination.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFPPIP%20OR%20FPPIP%29%20AND%20human)]

No publication is currently available.

## References

1 Zeng F., Southerland J.A., Voll R.J., Votaw J.R., Williams L., Ciliax B.J., Levey A.I., Goodman M.M. (2006). Synthesis and evaluation of two 18F-labeled imidazo[1,2-a]pyridine analogues as potential agents for imaging beta-amyloid in Alzheimer's disease. Bioorg Med Chem Lett.
2 Hardy J., Selkoe D.J. (2002). The amyloid hypothesis of Alzheimer's disease: progress and problems on the road to therapeutics. Science.
3 Wu C.Y., Pike V.W., Wang Y.M. (2005). Amyloid imaging: From benchtop to bedside. Current Topcis in Developmental Biology.
4 Masters C.L., Multhaup G., Simms G., Pottgiesser J., Martins R.N., Beyreuther K. (1985). Neuronal origin of a cerebral amyloid: neurofibrillary tangles of Alzheimer's disease contain the same protein as the amyloid of plaque cores and blood vessels. Embo J.
5 Kang J., Lemaire H.G., Unterbeck A., Salbaum J.M., Masters C.L., Grzeschik K.H., Multhaup G., Beyreuther K., Muller-Hill B. (1987). The precursor of Alzheimer's disease amyloid A4 protein resembles a cell-surface receptor. Nature.
6 Carter J., Lippa C.F. (2001). Beta-amyloid, neuronal death and Alzheimer's disease. Curr Mol Med.
7 Okamura N., Suemoto T., Shimadzu H., Suzuki M., Shiomitsu T., Akatsu H., Yamamoto T., Staufenbiel M., Yanai K., Arai H., Sasaki H., Kudo Y., Sawada T. (2004). Styrylbenzoxazole derivatives for in vivo imaging of amyloid plaques in the brain. J Neurosci.
8 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.